# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-rich Cys knot scaffold grafted with integrin α_v_β_6_-binding peptide RSLARTDLDHLRGR

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-rich Cys knot scaffolds grafted with integrin α_v_β_6_-binding peptide RSLARTDLDHLRGR
Abbreviated name: | ^64^Cu-DOTA-R_0_2
Synonym:
Backbone: | Peptide
Target: | Integrin α_v_β_6_
Mechanism: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_6_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Integrin α_v_β_6_ plays an important role in the development of epithelial cells and is nearly undetectable on adult normal tissues. However, the levels of α_v_β_6_ integrin can be upregulated during tissue remodeling and wound healing (11). On the other hand, α_v_β_6_ integrin is strongly expressed on tumor cells of the oral cavity, pancreas, breast, ovary, colon, and stomach (12-14). α_v_β_6_ integrin affects tumor growth, tumor invasiveness, and metastasis (13). α_v_β_6_ binds to the RGD motif in fibronectin, tenascin, and the viral protein 1 (VP1) of foot-and-mouth disease virus (FMDV) (15). FMDV binds to cells through the RGD motif of the GH loop of the VP1. A consensus α_v_β_6_-binding motif DLXXL was identified by using phage display screening with minimal binding to α_v_β_3_, α_IIb_β_3_, and α_v_β_5_ (16). Engineered cysteine knot peptides (knots) comprise a rigid molecular scaffold of ~4 kDa with three disulfide bonds and a centrally located β sheet. Kimura et al. (17) grafted a α_v_β_6_-binding peptide (RSLARTDLDHLRGR) into the loop 1 of an Arg-rich knot to produce the knot known as R_0_2, which was radiolabeled with ^64^Cu via 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugation to form ^64^Cu-DOTA-R_0_2 as a positron emission tomography (PET) probe for in vivo imaging of α_v_β_6_ integrin in tumor-bearing nude mice.

### Related Resource Links:

- Chapters in MICAD (knot peptide (http://www.ncbi.nlm.nih.gov/books?term=knot%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_6_ integrin (http://www.ncbi.nlm.nih.gov/gene/3694))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_6_ integrin (http://www.ncbi.nlm.nih.gov/omim/147558))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20synthesis)]

Kimura et al. (17) reported the synthesis of ^64^Cu-DOTA-R_0_2. R_0_2 was biosynthesized using Pichia pastoris. The N-terminus amine of R_0_2 was conjugated with DOTA-N-hydroxysuccinimide ester for labeling with ^64^Cu. The radiochemical purity was >95%, with a specific activity of 18.5 MBq/nmol (0.5 mCi/nmol) at the end of purification. The labeling yield was >80%. Molecular masses of R_0_2 (3.914 kDa) and DOTA-R_0_2 (4.296 kDa) were confirmed with matrix-assisted laser desorption/ionization-mass spectrometry. ^64^Cu-DOTA-R_0_2 remained >20% intact in mouse serum for 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28in%20vitro%20or%20cell%29)]

Competitive binding of soluble integrins α_v_β_6_, α_v_β_3_, α_v_β_5_, and α_5_β_1_ to yeast cells expressing R_0_2 was determined with flow cytometry (17). The binding affinity (K_d_) value for α_v_β_6_ was 3.2 ± 2.7 nM. Integrins α_v_β_3_, α_v_β_5_, and α_5_β_1_ (10–300 nM) exhibited little binding to R_0_2. Cellular accumulation of ^64^Cu-DOTA-R_0_2 was determined in A431 human epidermoid cancer and BxPC3 human pancreatic cancer cells (high α_v_β_6_ expression), and HEK293 human embryonic kidney cells (low α_v_β_6_ expression). A431 and BxPC3 cells exhibited one-fold higher radioactivity than that of HEK293 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20rodentia)]

Kimura et al. (17) performed biodistribution studies with 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-R_0_2 in nude mice (n = 3/group) bearing A431 xenografts. Data were obtained at 1 h and 24 h after injection. ^64^Cu-DOTA-R_0_2 had blood levels of 0.43% and 0.63% injected dose (ID)/g at 1 h and 24 h. The initial tracer accumulation in the α_v_β_6_-integrin-expressing A431 tumor was about 4.43% ID/g at 1 h and increased to 5.18% ID/g at 24 h. At 60 min, the highest radioactivity concentration was found in the kidney (115% ID/g), followed by the stomach (3.58% ID/g), liver (3.18% ID/g), lung (2.52% ID/g), and intestine (2.48% ID/g). The spleen, bone, muscle, skin, pancreas, and heart showed low levels of radioactivity (<1% ID/g). The tumor/muscle ratios were 10.31 and 8.45 at 1 h and 24 h, respectively. No blocking studies were performed.

^64^Cu-DOTA-R_0_2 PET imaging studies were performed in nude mice (n = 3) bearing both BxPC3 and HEK293 xenografts at 1, 2, 4, and 24 h after injection 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-R_0_2 (17). The BxPC3 tumors were clearly visualized as early as 1 h and as late as 24 h after injection. Major radioactivity was observed in the urinary bladder and kidneys. Region-of-interest analysis showed the tumor accumulation of ^64^Cu-DOTA-R_0_2 was 4.4 ± 0.7% ID/g in BxPC3 tumors compared with 1.3 ± 0.1% ID/g in HEK293 tumors. Average tumor/background ratios were ~9 (BxPC3) and ~2 (HEK293). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
12 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
13 Kawashima A., Tsugawa S., Boku A., Kobayashi M., Minamoto T., Nakanishi I., Oda Y. (2003). Expression of alphav integrin family in gastric carcinomas: increased alphavbeta6 is associated with lymph node metastasis. Pathol Res Pract.
14 Bates R.C. (2005). The alphaVbeta6 integrin as a novel molecular target for colorectal cancer. Future Oncol.
15 DiCara D., Rapisarda C., Sutcliffe J.L., Violette S.M., Weinreb P.H., Hart I.R., Howard M.J., Marshall J.F. (2007). Structure-function analysis of Arg-Gly-Asp helix motifs in alpha v beta 6 integrin ligands. J Biol Chem.
16 Kraft S., Diefenbach B., Mehta R., Jonczyk A., Luckenbach G.A., Goodman S.L. (1999). Definition of an unexpected ligand recognition motif for alphav beta6 integrin. J Biol Chem.
17 Kimura R.H., Teed R., Hackel B.J., Pysz M.A., Chuang C.Z., Sathirachinda A., Willmann J.K., Gambhir S.S. (2012). Pharmacokinetically stabilized cystine knot peptides that bind alpha-v-beta-6 integrin with single-digit nanomolar affinities for detection of pancreatic cancer. Clin Cancer Res.